# Gadolinium-tetraazacyclododecane tetraacetic acid coupled with folate via bis(aminoethyl)ethylene glycol linker

Chemical name: | Gadolinium-tetraazacyclododecane tetraacetic acid coupled with folate via bis(aminoethyl)ethylene glycol linker | [image]
Abbreviated name: | Gd.DOTA.Folate | [image]
Synonym: | | [image]
Agent Category: | Compounds | [image]
Target: | Folate receptor | [image]
Target Category: | Receptor | [image]
Method of detection: | Magnetic resonance imaging (MRI) | [image]
Source of signal / contrast: | Gadolinium (Gd^3+^) | [image]
Activation: | No | [image]
Studies: | - In vitro; - Rodents | Structure of Gd.DOTA.Folate (1).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=Folate%20Receptor%20and%20MRI)]

Gadolinium-tetraazacyclododecane tetraacetic acid (Gd.DOTA) coupled with folate via the bis(aminoethyl)ethylene glycol linker, abbreviated as Gd.DOTA. Folate, was synthesized by Kalber et al. for folate receptor (FR)-targeted magnetic resonance imaging (MRI) of FR-positive tumors (1).

Folate (folic acid) is an essential vitamin for cell synthesis of nucleotide bases. Cellular uptake of the folate is mediated either by membrane transport proteins or by FR. The human FR has three isoforms: FR-α-isoform, FR-β-isoform, and FR-γ-isoform. The FR-α isoform is expressed on the apical (luminal) surface of epithelial cells in limited tissues, and because of no vascular supply, it is inaccessible to exogenous folate conjugates with the exception of the FR-α isoforms on the proximal tubules of kidneys (1-3). The FR-β isoform is observed mainly on activated macrophages, whereas the FR-γ isoform is rarely detected in human tissues (1, 4). Several features of FR make it a valuable target for developing FR-targeted imaging and therapeutic agents (2, 3, 5). First, FR has a high affinity for the exogenous folate conjugates (K_d_ = ~100 pM), and the conjugates do not bind to most normal cells. Second, the FR-α isoform is overexpressed in ~40% of human cancer tissues, where it is completely accessible to folate conjugates. Third, folate conjugates are taken up by cancer cells via FR-mediated endocytosis, and FR recycles actively to the cell surface with a frequency of 5.7–20 h, depending on cell types. Fourth, conjugation of imaging labels via the γ-carboxyl group of folate has no apparent effects on the ligand-binding affinity to FR. Furthermore, folate is a small molecule (MW = ~441) and exhibits rapid and complete penetration of solid tumors and rapid clearance from FR-negative tissues (t_1/2_ = <10 min). However, the MRI contrast can be limited by the relatively low density of FR on the tumor cell surface (1–3 million FR/cell) and by the rapid saturation of binding (2, 3). Nevertheless, most studies demonstrate that cellular uptake of the Gd- or iron oxide-folate conjugates in FR-positive tumors is much higher than in FR-negative tumors. Normal organs except for the kidneys have minimal uptake (1, 2, 6).

Kalber et al. synthesized the novel compound Gd.DOTA.Folate by coupling folate to Gd.DOTA via bis(aminoethyl)ethylene glycol, a very short linker (1). MRI with Gd.DOTA.Folate in tumor-bearing mice showed an increase in R_1_ with clear enhancement on the MRI images in a human ovarian carcinoma (IGROV-1) xenograft overexpressing the FR-α isoform, but no change was observed in a FR-α–negative human ovarian carcinoma (OVCAR-3) xenograft. However, contrast enhancement with Gd.DOTA.Folate was not observed in vitro in either IGROV-1 cells or OVCAR-3 cells (i.e., the in vitro MRI data did not support the in vivo findings (1)). A similar discrepancy has been reported in other studies when comparing in vitro and in vivo results with FR-targeted agents (7, 8). Studies with ^153^Gd-folate dendrimer and P866 low molecular weight dimeric Gd.DOTA indicate that the discrepancy may be caused by the potential sensitivity limitation in vitro, perhaps due to the marked cellular variability in FR expression (5, 8). Miotti et al. have shown that the degree of internalized folate is not completely proportional to the degree of expression for the FR-α isoform because cell lines with low expression of the FR-α isoform are still capable of low levels of uptake (7). This appears to be supported by the in vitro studies by Kalber et al. in that, although the FR-α–positive IGROV-1 cells had a much higher degree of Gd.DOTA.Folate internalization than did the FR-α–negative OVCAR-3 cells, there was still a degree of uptake within the OVCAR-3 cells as measured with inductively coupled mass spectrometry (ICP-MS) (1).

### Related Resource Links:

- FR-targeted chapters (http://www.ncbi.nlm.nih.gov/books/?term=folate%20receptor%20AND%20micad%5bbook%5d) on MICAD
- Protein (http://www.ncbi.nlm.nih.gov/protein/?term=Folate+Receptor) and nucleotide (http://www.ncbi.nlm.nih.gov/nucleotide/?term=Folate+Receptor) information of FR
- FR-targeted clinical trials (http://clinicaltrials.gov/ct2/results?term=Folate+Receptor) in Clinicaltrials.gov

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/20809208)]

Kalber et al. described the details of Gd.DOTA.Folate synthesis (1). Solid-phase synthesis was utilized for the synthesis of the folate precursor (yield = 83%). The precursor was then reacted with activated DOTA-N-hydroxysuccinimide ester to produce the DOTA.Folate ligand (yield = 57%). Addition of Gd chloride to the ligand resulted in the target molecule, Gd.DOTA.Folate. The purity of Gd.DOTA.Folate was confirmed with high-performance liquid chromatography. The isotopic Gd peaks were clearly visible in the mass spectrometry. A xylenol orange assay did not indicate the presence of free Gd ions to any significant degree.

The MRI efficacy of Gd.DOTA.Folate in aqueous solution was measured, and a 70% reduction in the bulk water T_1_ value was observed compared to water alone and DOTA.Folate control solutions. The r_1_ relaxivity for Gd.DOTA.Folate was calculated to be 1.28 mM^-1^s^-1^, which was slightly lower than that of the non-conjugated Gd.DOTA (3.66 mM^-1^s^-1^) (1).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/20809208)]

In vitro MRI (4.7 T) was performed with agarose phantoms that contained cells obtained at 2, 8, and 14 h after incubation with 0.5 mM Gd.DOTA.Folate, DOTA.Folate, Gd.DOTA, or buffer alone (control) (1). Images did not show any signal enhancement or changes in R_1_ for any compound compared to control cells for either FR-α–positive IGROV-1 cells or FR-α–negative OVCAR-3 cells. However, ICP-MS studies of the cell pellets after 1 h incubation showed that IGROV-1 cells had a concentration of Gd that was approximately double that observed in the OVCAR-3 cells (P < 0.01), suggesting FR-α–mediated uptake in the IGROV-1 cells (1).

Competitive binding experiments were carried out with an excess of 1 mM folate that was added 15 min before the addition of Gd.DOTA.Folate (1). IGROV-1 cells showed a significant reduction in the Gd uptake (P < 0.01). OVCAR-3 cells also showed a reduction, although not to the same extent. Free folate did not completely inhibit the uptake of the folate conjugate in either cell line, suggesting that another mechanism of uptake rather than FR-mediated endocytosis also took place in both cell lines.

None of the agents (Gd.DOTA.Folate, DOTA.Folate, Gd.DOTA) had a significant effect on cell viability (1).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/20809208)]

In vivo MRI was performed in mice bearing either IGROV-1 or OVCAR-3 tumor xenografts at 2 h and 14 h after administration of Gd.DOTA.Folate, Gd.DOTA, or DOTA.Folate (control) (n = 3 mice/group) (1). MRI images with Gd.DOTA.Folate showed clear tumor enhancement in the IGROV-1 tumor xenografts compared to the baseline image, whereas OVCAR-3 tumor xenografts did not show any enhancement on the images. This observation was reflected in the R_1_ values. An increase in the R_1_ value was observed at 2 h in the IGROV-1 tumors, and this value increased further at 14 h (P < 0.05). No change in the R_1_ values was noted with any of the other groups. The gradual increase in R_1_ values over the 14 h in the IGROV-1 mice treated with Gd.DOTA.Folate suggests that the compound is not washed out of the tumor over this time period; consequently, the compound is either bound to the FR or internalized into the tumor cells through the receptor-mediated transportation. Liver and kidneys showed a slight increase in R_1_ values; however, the results were not significant, and MRI images were not consistently enhanced in all animals (data not shown).

The presence of Gd within the IGROV-1 tumors in mice treated with Gd.DOTA.Folate was confirmed at 14 h with laser ablation-ICP-MS (1). ^157^Gd was mainly situated in the rim of the tumor. No ^157^Gd was detected in the necrotic areas of the tumor core or in tumors from mice injected with the Gd-free control agent, DOTA.Folate. Blocking studies were not reported.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28primate%20NOT%20human%29)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20human)]

No references are currently available.

## References

1 Kalber, T.L., N. Kamaly, P.W. So, J.A. Pugh, J. Bunch, C.W. McLeod, M.R. Jorgensen, A.D. Miller, and J.D. Bell, A Low Molecular Weight Folate Receptor Targeted Contrast Agent for Magnetic Resonance Tumor Imaging. Mol Imaging Biol, 2010
2 Sega E.I., Low P.S. (2008). Tumor detection using folate receptor-targeted imaging agents. Cancer Metastasis Rev.
3 Low P.S., Kularatne S.A. (2009). Folate-targeted therapeutic and imaging agents for cancer. Curr Opin Chem Biol.
4 Low P.S., Henne W.A., Doorneweerd D.D. (2008). Discovery and development of folic-acid-based receptor targeting for imaging and therapy of cancer and inflammatory diseases. Acc Chem Res.
5 Zhao X., Li H., Lee R.J. (2008). Targeted drug delivery via folate receptors. Expert Opin Drug Deliv.
6 Wang Z.J., Boddington S., Wendland M., Meier R., Corot C., Daldrup-Link H. (2008). MR imaging of ovarian tumors using folate-receptor-targeted contrast agents. Pediatr Radiol.
7 Miotti S., Bagnoli M., Ottone F., Tomassetti A., Colnaghi M.I., Canevari S. (1997). Simultaneous activity of two different mechanisms of folate transport in ovarian carcinoma cell lines. J Cell Biochem.
8 Konda S.D., Aref M., Wang S., Brechbiel M., Wiener E.C. (2001). Specific targeting of folate-dendrimer MRI contrast agents to the high affinity folate receptor expressed in ovarian tumor xenografts. MAGMA.